# ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-iron oxide-c(RGDyK) nanoparticles

Chemical name: | ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-iron oxide-c(RGDyK) nanoparticles
Abbreviated name: | ^64^Cu-DOTA-IO-RGDyK
Synonym:
Agent category: | Peptide
Target: | Integrin α_v_β_3_
Target category: | Receptor-ligand binding
Method of detection: | Positron emission tomography (PET), magnetic resonance imaging (MRI)
Source of signal: | ^64^Cu and iron oxide
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&val=4504763), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nucleotide&val=40217844) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=3685) for more information about integrin α_v_β_3_.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Iron+oxide+RGD)]

Magnetic resonance imaging (MRI) maps information about tissues spatially and functionally. Protons (hydrogen nuclei) are widely used in imaging because of their abundance in water molecules. Water comprises ~80% of most soft tissue. The contrast of proton MRI depends primarily on the density of the nucleus (proton spins), the relaxation times of the nuclear magnetization (T_1_, longitudinal, and T_2_, transverse), the magnetic environment of the tissues, and the blood flow to the tissues. However, insufficient contrast between normal and diseased tissues requires the use of contrast agents. Most contrast agents affect the T_1_ and T_2_ relaxation times of the surrounding nuclei, mainly the protons of water. T_2_* is the spin–spin relaxation time composed of variations from molecular interactions and intrinsic magnetic heterogeneities of tissues in the magnetic field (1). Cross-linked iron oxide (CLIO) nanoparticles and other iron oxide formulations affect T_2_ primarily and lead to decreased signals. On the other hand, the paramagnetic T_1_ agents, such as gadolinium (Gd^3+^) and manganese (Mn^2+^), accelerate T_1_ relaxation and lead to brighter contrast images.

Integrins are a family of heterodimeric glycoproteins on cell surfaces that mediate diverse biological events involving cell–cell and cell–matrix interactions (2). Integrins consist of an α and a β subunit and are important for cell adhesion and signal transduction. The α_v_β_3_ integrin is the most prominent receptor class affecting tumor growth, tumor invasiveness, metastasis, tumor-induced angiogenesis, inflammation, osteoporosis, and rheumatoid arthritis (3-8). The α_v_β_3_ integrin is strongly expressed on tumor cells and activated endothelial cells. In contrast, expression of α_v_β_3_ integrin is weak on resting endothelial cells and most normal tissues. The α_v_β_3_ antagonists are being studied as antitumor and antiangiogenic agents, and the agonists are being studied as angiogenic agents for coronary angiogenesis (7, 9, 10). The tripeptide sequence Arg-Gly-Asp (RGD) is identified as a recognition motif used by extracellular matrix proteins (vitronectin, fibrinogen, laminin, and collagen) to bind to a variety of integrins including α_v_β_3_. Various radiolabeled cyclic RGD peptides have been introduced for imaging of tumors and tumor angiogenesis (11). ^64^Cu-1,4,7,10-Tetraazacyclododecane-N,N’,N’’,N’’’-tetraacetic acid-iron oxide-c(RGDyK) (^64^Cu-DOTA-IO-RGDyK) nanoparticles have been developed as a multimodality probe for positron emission tomography (PET) and MRI of tumor vasculature to study in vivo biodistribution of the tracer in tumor-bearing mice (12). ^64^Cu-DOTA-IO-RGDyK has been shown to have a high accumulation in the tumor vasculature with little extravastion and predominant liver and spleen accumulation.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Iron+oxide+RGD+synthesis)]

Polyaspartic acid (PASP, 0.3 mmol) in ammonia was added to 0.6 M FeCl_3_ and 0.3 M FeCl_2_. The mixture was heated for 1 h at 100°C (12). PASP-Coated nanoparticles were purified with dialysis. DOTA was activated with ethyl-3-dimethylaminopropyl-carbodiimide and sulfo-N-hydroxysuccinimide for 30 min. The activated DOTA (800 nmol) and the bifunctional linker NHS-poly(ethylene glycol-maleimide (1,200 nmol) were added to a solution of PASP-coated nanoparticles (0.039 mmol iron concentration). The mixture was incubated for 60 min at 4°C. c(RGDyK)-SH (1,500 nmol) was incubated with the mixture overnight at room temperature. DOTA-IO-RGDyK nanoparticles were purified with column chromatography and dialysis. DOTA-IO-RGDyK nanoparticles and ^64^CuCl_2_ in acetate buffer (pH 6.5) were incubated for 40 min at 40°C. ^64^Cu-DOTA-IO-RGDyK nanoparticles were isolated with column chromatography. The average size of DOTA-IO-RGDyK nanoparticles was 45 ± 10 nm in buffer as measured with transmission electron microscope. Each particle contained ~35 c(RGDyK) molecules and ~30 DOTA-chelating groups. ^64^Cu-DOTA-IO-RGDyK nanoparticles had a specific activity of 185 GBq/g of iron (5 Ci/g of iron).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Iron+oxide+RGD+in%20vitro)]

Lee et al. (12) performed a competitive cell-binding assay using human glioblastoma U87MG tumor cells (expressing α_v_β_3_). DOTA-IO-RGDyK nanoparticles inhibited the binding of ^125^I-echistatin in a dose-dependent manner with a 50% inhibition concentration of 34 ± 5 nM, which was ~6-fold lower than that of c(RGDyK). DOTA-IO nanoparticles had no inhibitory effect on the binding assay. IO nanoparticles exhibited a T_2_ relaxivity r_2_ value (at 3 T) of 105.5 mM^-1^s^-1^, whereas ferumoxide exhibited a r_2_ value of 151.9 mM^-1^ s^-1^.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Iron+oxide+RGD+rodentia)]

Lee et al. (12) used a whole-body PET imaging system to study the accumulation of 3.7 MBq (0.1 mCi) ^64^Cu-DOTA-IO-c(RGDyK) or ^64^Cu-DOTA-IO in nude mice bearing U87MG tumors. ^64^Cu-DOTA-IO-c(RGDyK) (300 µg of iron) was injected intravenously into tumor-bearing mice (n = 3/group). Tumor accumulation of ^64^Cu-DOTA-IO-c(RGDyK) was 7.9% injected dose/gram (ID/g) at 1 h, 10.1% ID/g at 4 h, and 9.8% ID/g at 21 h. ^64^Cu-DOTA-IO showed tumor accumulation of <5% ID/g at these time points. There was no difference in accumulation at 4 h in the liver (23% ID/g) and kidney (5% ID/g) between the two nanoparticles. Co-injection of c(RGDyK) (10 mg/kg) with ^64^Cu-DOTA-IO-c(RGDyK) reduced the tumor radioactivity levels to <4% ID/g at these time points. T_2_-Weighted MRI studies at 3 T were performed in mice bearing U87MG tumors after intravenous injection of DOTA-IO-c(RGDyK) nanoparticles. There was a greater tumor signal reduction in the mice receiving DOTA-IO-c(RGDyK) nanoparticles as compared with that in mice receiving DOTA-IO nanoparticles or co-injection of DOTA-IO-RGDyK at 4 h after injection. The strong contrast reduction was similar in the liver and spleen for both nanoparticles. Staining of iron in tissue sections confirmed the MRI findings.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Iron+oxide+RGD+and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Iron+oxide+RGD+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Iron+oxide+RGD+human)]

No publication is currently available.

## NIH Support

R24 CA93862, P50 CA114747, R01 CA119053, R21 CA102123, R21 CA121842, U54 CA119367

## References

1 Wang Y.X., Hussain S.M., Krestin G.P. (2001). Superparamagnetic iron oxide contrast agents: physicochemical characteristics and applications in MR imaging. Eur Radiol.
2 Hynes R.O. (1992). Integrins: versatility, modulation, and signaling in cell adhesion. Cell.
3 Jin H., Varner J. (2004). Integrins: roles in cancer development and as treatment targets. Br J Cancer.
4 Varner J.A., Cheresh D.A. (1996). Tumor angiogenesis and the role of vascular cell integrin alphavbeta3. Important Adv Oncol.
5 Wilder R.L. (2002). Integrin alpha V beta 3 as a target for treatment of rheumatoid arthritis and related rheumatic diseases. Ann Rheum Dis.
6 Grzesik W.J. (1997). Integrins and bone--cell adhesion and beyond. Arch Immunol Ther Exp (Warsz).
7 Kumar C.C. (2003). Integrin alpha v beta 3 as a therapeutic target for blocking tumor-induced angiogenesis. Curr Drug Targets.
8 Ruegg C., Dormond O., Foletti A. (2002). Suppression of tumor angiogenesis through the inhibition of integrin function and signaling in endothelial cells: which side to target?. Endothelium.
9 Kerr J.S., Mousa S.A., Slee A.M. (2001). Alpha(v)beta(3) integrin in angiogenesis and restenosis. Drug News Perspect.
10 Mousa S.A. (2003). alphav Vitronectin receptors in vascular-mediated disorders. Med Res Rev.
11 Haubner R., Wester H.J. (2004). Radiolabeled tracers for imaging of tumor angiogenesis and evaluation of anti-angiogenic therapies. Curr Pharm Des.
12 Lee H.Y., Li Z., Chen K., Hsu A.R., Xu C., Xie J., Sun S., Chen X. (2008). PET/MRI dual-modality tumor imaging using arginine-glycine-aspartic (RGD)-conjugated radiolabeled iron oxide nanoparticles. J Nucl Med.